# 3-[2-[4-(4-[^18^F]Fluorobenzoyl)-1-piperidyl]ethyl]-2-sulfanyl-3H-quinazolin-4-one

Chemical name: | 3-[2-[4-(4-[^18^F]Fluorobenzoyl)-1-piperidyl]ethyl]-2-sulfanyl-3H-quinazolin-4-one
Abbreviated name:
Synonym: | [^18^F]Altanserin
Agent Category: | Compound
Target: | 5-HT_2A_ serotonin receptors
Target Category: | Receptor binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem.

## Background

[P ubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Altanserin)]

Serotonin (5-hydroxytryptamine, 5-HT) has diverse physiologic roles as a neurotransmitter in the central nervous system (1). It is involved in regulation and modulation of sleep, affective and personality behaviors, and pain. It also is a regulator of smooth muscle function and platelet aggregation. The brain cortical 5-HT system has been implicated in several neuropsychiatric disorders, including major depression, anxiety, obsessive-compulsive disorder, and schizophrenia (2, 3). The effects of 5-HT are mediated by as many as seven classes of receptor populations (5-HT_1_ to 5-HT_7_), many of which include several subtypes (4). There are three receptor subtypes within the G protein-coupled 5-HT_2_ receptor family: 5-HT_2A_, 5-HT_2B_, and 5-HT_2C_.

5-HT_2A_ receptors are abundantly present in the cerebral cortex, basal forebrain, hippocampus, amygdala, dorsal thalamus, hypothalamus, superior colliculus, substantia nigra, pedunculopontine nucleus, legmental area, and myelencephalon (5). 5-HT_2A_ receptors are involved in mediation of normal and psychotic states, working memory, regulation of GABAergic and cholinergic neuronal cells, sleep, peripheral pain, and cardiovascular functions. 5-HT_2B_ receptors are found mainly in several peripheral tissues, such as the stomach, intestine, and pulmonary smooth muscle, and in the myocardium. In the brain, 5-HT_2B_ receptors are found in discrete nuclei of the cerebellum, lateral septum, dorsal hypothalamus, dorsal raphe, and amygdala. 5-HT_2C_ receptors are found in the choroid plexus, substantia nigra, globus pallidus, and ventromedial thalamus. 5-HT_2A_ receptors are implicated in several psychiatric disorders, such as schizophrenia, depression, and obsessive-compulsive disorder. Thus, there is a need for selective ligands to investigate the pharmacologic role of 5-HT_2A_ receptors.

There have been several studies to develop specific 5-HT_2A_ radioligands, such as [^11^C]ketanserin (6), [^18^F]spiperone (7), [^11^C]methylspiperone ([^11^C]NMSP), and [^18^F]setoperone [PubMed], for positron emission tomography (PET) imaging. However, none has proven specific for 5-HT_2A_ receptors because these compounds also bind to other receptors, such as dopamine receptors and 5-HT_1_ receptor subtypes. Altanserin, a fluorobenzoyl derivative related to ketanserin, was reported to be a potent inhibitor of 5-HT_2A_ receptors with >100-fold selectivity over D_2/3_ receptors, 5-HT_1A_, 5-HT_6_, and 5-HT_7_ (8, 9). This led to the development of 3-[2-[4-(4-[^18^F]fluorobenzoyl)-1-piperidyl]ethyl]-2-sulfanyl-3H-quinazolin-4-one ([^18^F]altanserin) as a useful tool for 5-HT_2A_ receptor PET imaging in vivo (10).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=altanserin%20and%20synthesis)]

The reported radiosynthesis of [^18^F]altanserin involved nucleophilic substitution of 3-[2-[4-(4-nitrobenzoyl)-1-piperidyl]ethyl]-2-sulfanyl-3H-quinazolin-4-one with K[^18^F]F/Kryptofix2.2.2 in dimethyl sulfoxide, followed by high-performance liquid chromatography (HPLC) purification (10). The reported overall radiochemical yield of the radiosynthesis was 10% at end of synthesis (EOS), the specific radioactivity was 30-48 GBq/µmol (0.8-1.3 Ci/µmol), and the radiochemical purity was >99%. The time for synthesis and purification was approximately 110 min.

Monclus et al. (11) and Tan et al. (12) reported automatic systems for synthesis of [^18^F]altanserin using microwave heating and SepPak and HPLC purification. [^18^F]Altanserin was prepared in 90-114 min with 20% radiochemical yield, a radiochemical purity >99%, and specific radioactivity of 103-115 GBq/µmol (2.8-3.1 Ci/µmol) at EOS.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=altanserin%20and%20in%20vitro)]

Altanserin has been reported to have high binding affinities for 5-HT_2A_ receptor sites. Leysen (8) reported K_i_ values for 5-HT_2A_, 5-HT_1A,_ D_2_, α_1_, and H_1_ receptors of 0.13, 1400, 62, 4.6, and 7.8 nM, respectively. Tan et al. (9) extended the studies, obtaining K_i_ values for 5-HT_2A_, 5-HT_2c_, 5-HT_6_, and 5-HT_7_ of 0.3, 6, 1756, and 15 nM, respectively. They also found that the binding of 4-(4-fluorobenzoyl)piperidine (4-FBP) and altanserinol, the major plasma metabolites of altanserin, to these four 5-HT receptor subtypes was negligible. These data support that altanserin is a specific 5-HT_2A_ antagonist.

In vitro studies of [^18^F]altanserin binding produced K_d_ values of 0.30, 0.24, and 0.33 nM for rat cerebrum, frontal cortex, and cerebellum, respectively (13). The 5-HT_2A_B_max_ values were 145, 523, and 8 fmol/mg protein for rat cerebrum, frontal cortex, and cerebellum, respectively. In saturation binding studies using [^18^F]altanserin, the estimated K_d_ value was 0.28 ± 0.03 nM (0.35 ± 0.04 nM with 100 nM SB 206553, a selective 5-HT_2B/C_ antagonist) for rat frontal cortex membranes. The B_max_ values were 153 ± 5 and 156 ± 10 fmol/mg protein without and with 100 nM SB 206553, respectively. Similarly, the K_d_ and B_max_ were almost the same in the presence or absence of prazosin, a selective α_1_-receptor antagonist.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=altanserin%20and%20rodentia)]

Biodistribution studies in rats showed a moderate accumulation of radioactivity in the whole brain with 0.42%, 0.54%, and 0.21% injected dose (ID)/g, respectively, at 5, 60, and 240 min after injection of [^18^F]altanserin (10). There was a marked accumulation of the tracer in the frontal cortex within the first 5 min (1.14% ID/g), followed by a slow decrease of radioactivity to 1.00% ID/g at 60 min. The striatum (0.39% ID/g) and thalamus (0.18% ID/g) exhibited slightly lower radioactivity compared with the frontal cortex at 60 min. The maximum frontal cortex-to-cerebellum, striatum-to-cerebellum, and thalamus-to-cerebellum ratios were 10.8, 3.6, and 1.8, respectively, at 120 min. The bulk of accumulation was in the lungs, liver, and kidneys at 5 min. Clearance of radioactivity occurred at 240 min for all tissues except the bone, which showed an increase from 0.18% ID/g at 5 min to 0.31% ID/g at 240 min, most likely because of defluorination. The accumulation of [^18^F]altanserin in frontal cortex and striatum was blocked by various unlabeled 5-HT_2_ antagonists (ketanserin, mesulergin, ritanserin, and spiperone) but not by D_2_ antagonists (sulpiride and halopemide). The fraction of unchanged [^18^F]altanserin in blood samples determined by HPLC was 85%, and [^18^F]altanserin remained 96% intact in the brain at 240 min after injection.

In an autoradiographic study of in vivo binding of [^18^F]altanserin in rat brain, the highest levels were found in the frontal cortex, claustrum, and anterior olfactory nuclei (14). [^18^F]Altanserin binding to the frontal cortex was reversed (59%) by administration of ketanserin (4 mg/kg) 30 min after tracer injection. Ketanserin (4 mg/kg) and mesulergin (10 mg/kg) pretreatment blocked [^18^F]altanserin binding by 82% and 85%, respectively. On the other hand, sulpiride and prazosin showed no significant inhibition. The B_max_ values for the frontal cortex were estimated to be 36.7 ± 3.4 and 30.2 ± 4.2 pmol/g tissue by electronic and film optical counting, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20altanserin%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=altanserin%20and%20%28primate%20not%20human%29)]

[^18^F]Altanserin was administered to baboons by bolus (170 MBq, or 4.6 mCi) plus constant infusion (41 MBq/h, or 1.1 mCi/h) (15). PET measurements began after the plasma level was stabilized, by 4-5 h after injection. High accumulation of [^18^F]altanserin was found in the cortical regions of baboon brains, with nonsignificant levels in the striatum and cerebellum at 8 h. [^18^F]Altanserin binding to the frontal cortex was reversed (73 ± 13%) by administration of ketanserin (1.5-2.0 mg/kg) 5.5-6.5 h after the tracer injection, whereas there was only a 6 ± 2% decrease in the cerebellum. Injection of 1.5 mg/kg SR46349B (another 5-HT_2A_ antagonist) resulted in a 76% decrease in the cortical region, but only a 13% decrease in the cerebellum, a tissue thought to have very low density of 5-HT_2A_ receptors.

The brain accumulation of radioactivity was studied by PET imaging in baboons after bolus injection of [^18^F]altanserin, [^18^F]altanserinol, or [^18^F]4-FBP, with accumulations in the frontal cortex of 0.014%, 0.004%, and 0.010% ID/ml, respectively, at 25 min (16). [^18^F]Altanserin images (35-90 min post injection) displayed radioactivity concentrations that followed a rank order: frontal and temporal cortices > thalamus > basal ganglia > cerebellum. Regionally, specific 5-HT_2A_ receptor binding was not evident in the later [^18^F]altanserinol or [^18^F]4-FBP image data. These data were consistent with blood-brain barrier passage and nonspecific localization of [^18^F]altanserinol, [^18^F]4-FBP, and/or their secondary radiolabeled metabolites. Therefore, the uniformity of nonspecific binding of these metabolites in all brain regions strengthened the validity of analyses of [^18^F]altanserin PET data by conventional methods of kinetic rate constants. After bolus injection of [^18^F]altanserin in baboons, 88 ± 5% and 23 ± 8% of the total plasma radioactivity was intact [^18^F]altanserin at 2 and 90 min, respectively. [^18^F]Altanserinol and [^18^F]4-FBP were 12% and 50% at 90 min. In contrast, no major metabolites of [^18^F]altanserin were found in rat plasma and brain (10).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=altanserin%20and%20human)]

[^18^F]Altanserin PET studies of 5-HT_2A_ receptor distribution in human brain have shown a significant major localization of radioactivity in the cortical regions and a minor accumulation in the striatal regions (17-19). Quantitative analysis of [^18^F]altanserin binding was usually performed using distribution volume (DV) and/or kinetic rate constants (Logan graphic method) from which binding potential (BP; k_3_/k_4_ or B_max_/K_d_) was derived to measure receptor concentrations. Biver et al. (17) reported on [^18^F]altanserin PET studies in 12 healthy subjects (27-45 years of age). PET brain scans showed high accumulation of radioactivity in the cortical regions (temporal > frontal > parietal > limbic > occipital) at 90 min after injection of [^18^F]altanserin (3.7 MBq/kg, or 0.1 mCi/kg). Accumulations in the basal ganglia and cerebellum were very low. The frontal cortex-to-cerebellum ratio was about 2.4. The frontal cortex BP was 2.98 ± 0.917 and 2.97 ± 0.679 by nonlinear regression and Logan graphic analysis, respectively. At 90 min post injection, 45% of [^18^F]altanserin radioactivity remained intact in plasma. In a later study, Price et al. (20) concluded that the most comprehensive and quantitatively valid analysis for bolus [^18^F]altanserin PET data was the dual-input method, which specifically accounted for blood-brain barrier-permeable metabolites, although the Logan graphic method was preferred because it provided a good compromise between validity, sensitivity, and reliability of implementation. Sadzot et al. (18) showed that ketanserin (0.1 mg/kg) was able to displace [^18^F]altanserin binding in all brain regions when administered 57 min after the tracer injection. Smith et al. (19) demonstrated good test-retest reliability of [^18^F]altanserin Logan DV values in various brain regions.

Meltzer et al. (21) studied the effects of age on the binding of [^18^F]altanserin to 5-HT_2A_ receptor sites in 9 healthy elderly (ages 61-76 years) and 9 healthy young (ages 18-29 years) subjects by PET imaging. The BPs of the 5-HT_2A_ receptors in the striatum, cingulate, amygdala/hippocampus, occipital cortex, and temporal cortex decreased with age by 49%, 65%, 66%, 47%, and 58%, respectively. In another study with 22 healthy subjects (21-69 years of age), Sheline et al. (22) found an age-dependent decrease of 5-HT_2A_ receptor BP (about 17% per decade) in the hippocampus, cingulate occipital cortex, prefrontal cortex, and occipital cortex. The 5-HT_2A_ receptor loss was progressive from the second decade through the fifth decade (70% loss) and then leveled off. Adams et al. (23) reported, in a study of 52 healthy subjects (ages 21-79 years), that there were significant negative correlations between all cortical regions, except the occipital cortex, in 5-HT_2A_ receptor binding (measured as specific DV, with cerebellum as the reference) and age, with a loss of 6% per decade. The DVs of the caudate, putamen, and thalamus were also unrelated to age. On the other hand, there was a positive correlation between cerebellar 5-HT_2A_ receptor binding and age. There was no difference in 5-HT_2A_ DV between men and women.

Studies have found significant reductions in 5-HT_2A_ BPs in the orbito-insular cortex (24) and hippocampus (25, 26) of patients with depression but free of any psychotropic medication for at least 10 days. There were some decreases in BP in other cortical regions, but these were not significant. In Alzheimer’s disease (27), anorexia nervosa (28, 29), and schizophrenia (30) patients (free of psychotropic medications), there were significant decreases in 5-HT_2A_ receptor binding in various cortical regions. On the other hand, there was a significant increase in 5-HT_2A_ BP in the caudate nuclei in patients with obsessive-compulsive disorder compared with healthy control subjects (31).

[^18^F]Altanserin PET is useful for objective monitoring of 5-HT_2A_ receptor density in patients with psychological disorders. Internal dosimetry data for [^18^F]altanserin in humans are not available in the literature.

## NIH Support

AG5133, MH52247, MH49936, MH01210, MH55305, MH30929, MH58620, P50 DA84733, MH58444, MH01370, MH54731, K24 MH6542, RR00036, MH49936, MH00295

## References

1 Lucki I. (1998). The spectrum of behaviors influenced by serotonin. Biol Psychiatry.
2 Fletcher A., Cliffe I.A., Dourish C.T. (1993). Silent 5-HT1A receptor antagonists: utility as research tools and therapeutic agents. Trends Pharmacol Sci.
3 Hoyer D., Clarke D.E., Fozard J.R., Hartig P.R., Martin G.R., Mylecharane E.J., Saxena P.R., Humphrey P.P. (1994). International Union of Pharmacology classification of receptors for 5-hydroxytryptamine (Serotonin). Pharmacol Rev.
4 Lanfumey L., Hamon M. (2004). 5-HT1 receptors. Curr Drug Targets CNS Neurol Disord.
5 Leysen J.E. (2004). 5-HT2 receptors. Curr Drug Targets CNS Neurol Disord.
6 Dewey S.L., Smith G.S., Logan J., Brodie J.D. (1993). Modulation of central cholinergic activity by GABA and serotonin: PET studies with 11C-benztropine in primates. Neuropsychopharmacology.
7 Shiue C.Y., Fowler J.S., Wolf A.P., Watanabe M., Arnett C.D. (1985). Syntheses and specific activity determinations of no-carrier-added (NCA) F-18-labeled butyrophenone neuroleptics--benperidol, haloperidol, spiroperidol, and pipamperone. J Nucl Med.
8. Leysen, J., Use of 5-HT receptor agonists and antagonists for the characterization of their respective recptor sites. In: A.B. Boulton, G.B. Baker and A.V. Jurio Editors, Drugs as Tools in Neurotransmitter Research. Neuromethods The Human Press, Clifton, NJ 1989: p. 299-341.
9 Tan P.Z., Baldwin R.M., Van Dyck C.H., Al-Tikriti M., Roth B., Khan N., Charney D.S., Innis R.B. (1999). Characterization of radioactive metabolites of 5-HT2A receptor PET ligand [18F]altanserin in human and rodent. Nucl Med Biol.
10 Lemaire C., Cantineau R., Guillaume M., Plenevaux A., Christiaens L. (1991). Fluorine-18-altanserin: a radioligand for the study of serotonin receptors with PET: radiolabeling and in vivo biologic behavior in rats. J Nucl Med.
11 Monclus M., Van Naemen J., Mulleneers E., Damhaut P., Luxen A., Goldman S. (1998). Automatic Synthesis of [(18)F]Altanserin, a Radiopharmaceutical for Positron Emission Tomographic Studies of the Serotonergic Type-2 Receptors. Clin Positron Imaging.
12 Tan P.Z., Baldwin R.M., Soufer R., Garg P.K., Charney D.S., Innis R.B. (1999). A complete remote-control system for reliable preparation of [18F]altanserin. Appl Radiat Isot.
13 Kristiansen H., Elfving B., Plenge P., Pinborg L.H., Gillings N., Knudsen G.M. (2005). Binding characteristics of the 5-HT(2A) receptor antagonists altanserin and MDL 100907. Synapse.
14 Biver F., Lotstra F., Monclus M., Dethy S., Damhaut P., Wikler D., Luxen A., Goldman S. (1997). In vivo binding of [18F]altanserin to rat brain 5HT2 receptors: a film and electronic autoradiographic study. Nucl Med Biol.
15 Staley J.K., Van Dyck C.H., Tan P.Z., Al Tikriti M., Ramsby Q., Klump H., Ng C., Garg P., Soufer R., Baldwin R.M., Innis R.B. (2001). Comparison of [(18)F]altanserin and [(18)F]deuteroaltanserin for PET imaging of serotonin(2A) receptors in baboon brain: pharmacological studies. Nucl Med Biol.
16 Price J.C., Lopresti B.J., Mason N.S., Holt D.P., Huang Y., Mathis C.A. (2001). Analyses of [(18)F] altanserin bolus injection PET data. I: consideration of radiolabeled metabolites in baboons. Synapse.
17 Biver F., Goldman S., Luxen A., Monclus M., Forestini M., Mendlewicz J., Lotstra F. (1994). Multicompartmental study of fluorine-18 altanserin binding to brain 5HT2 receptors in humans using positron emission tomography. Eur J Nucl Med.
18 Sadzot B., Lemaire C., Maquet P., Salmon E., Plenevaux A., Degueldre C., Hermanne J.P., Guillaume M., Cantineau R., Comar D., Franck G. (1995). Serotonin 5HT2 receptor imaging in the human brain using positron emission tomography and a new radioligand, [18F]altanserin: results in young normal controls. J Cereb Blood Flow Metab.
19 Smith G.S., Price J.C., Lopresti B.J., Huang Y., Simpson N., Holt D., Mason N.S., Meltzer C.C., Sweet R.A., Nichols T., Sashin D., Mathis C.A. (1998). Test-retest variability of serotonin 5-HT2A receptor binding measured with positron emission tomography and [18F]altanserin in the human brain. Synapse.
20 Price J.C., Lopresti B.J., Meltzer C.C., Smith G.S., Mason N.S., Huang Y., Holt D.P., Gunn R.N., Mathis C.A. (2001). Analyses of [(18)F]altanserin bolus injection PET data. II: consideration of radiolabeled metabolites in humans. Synapse.
21 Meltzer C.C., Smith G., Price J.C., Reynolds C.F., Mathis C.A., Greer P., Lopresti B., Mintun M.A., Pollock B.G., Ben-Eliezer D., Cantwell M.N., Kaye W., DeKosky S.T. (1998). Reduced binding of [18F]altanserin to serotonin type 2A receptors in aging: persistence of effect after partial volume correction. Brain Res.
22 Sheline Y.I., Mintun M.A., Moerlein S.M., Snyder A.Z. (2002). Greater loss of 5-HT(2A) receptors in midlife than in late life. Am J Psychiatry.
23 Adams K.H., Pinborg L.H., Svarer C., Hasselbalch S.G., Holm S., Haugbol S., Madsen K., Frokjaer V., Martiny L., Paulson O.B., Knudsen G.M. (2004). A database of [(18)F]-altanserin binding to 5-HT(2A) receptors in normal volunteers: normative data and relationship to physiological and demographic variables. Neuroimage.
24 Biver F., Wikler D., Lotstra F., Damhaut P., Goldman S., Mendlewicz J. (1997). Serotonin 5-HT2 receptor imaging in major depression: focal changes in orbito-insular cortex. Br J Psychiatry.
25 Mintun M.A., Sheline Y.I., Moerlein S.M., Vlassenko A.G., Huang Y., Snyder A.Z. (2004). Decreased hippocampal 5-HT2A receptor binding in major depressive disorder: in vivo measurement with [18F]altanserin positron emission tomography. Biol Psychiatry.
26 Sheline Y.I., Mintun M.A., Barch D.M., Wilkins C., Snyder A.Z., Moerlein S.M. (2004). Decreased hippocampal 5-HT(2A) receptor binding in older depressed patients using [18F]altanserin positron emission tomography. Neuropsychopharmacology.
27 Meltzer C.C., Price J.C., Mathis C.A., Greer P.J., Cantwell M.N., Houck P.R., Mulsant B.H., Ben-Eliezer D., Lopresti B., DeKosky S.T., Reynolds C.F. (1999). PET imaging of serotonin type 2A receptors in late-life neuropsychiatric disorders. Am J Psychiatry.
28 Bailer U.F., Price J.C., Meltzer C.C., Mathis C.A., Frank G.K., Weissfeld L., McConaha C.W., Henry S.E., Brooks-Achenbach S., Barbarich N.C., Kaye W.H. (2004). Altered 5-HT(2A) receptor binding after recovery from bulimia-type anorexia nervosa: relationships to harm avoidance and drive for thinness. Neuropsychopharmacology.
29 Frank G.K., Kaye W.H., Meltzer C.C., Price J.C., Greer P., McConaha C., Skovira K. (2002). Reduced 5-HT2A receptor binding after recovery from anorexia nervosa. Biol Psychiatry.
30 Hurlemann R., Boy C., Meyer P.T., Scherk H., Wagner M., Herzog H., Coenen H.H., Vogeley K., Falkai P., Zilles K., Maier W., Bauer A. (2005). Decreased prefrontal 5-HT(2A) receptor binding in subjects at enhanced risk for schizophrenia. Anat Embryol (Berl).
31 Adams K.H., Hansen E.S., Pinborg L.H., Hasselbalch S.G., Svarer C., Holm S., Bolwig T.G., Knudsen G.M. (2005). Patients with obsessive-compulsive disorder have increased 5-HT2A receptor binding in the caudate nuclei. Int J Neuropsychopharmacol.